# ^131^I-Chlorotoxin

Chemical name: | ^131^I-Chlorotoxin
Abbreviated name: | ^131^I-TM-601
Synonym: | Cltx
Agent Category: | Peptide
Target: | Matrix metalloproteinase 2 (MMP2) receptor
Target Category: | Ligand-receptor binding
Method of detection: | SPECT
Source of signal: | ^131^I
Activation: | Not required
Studies: | - Rodents; - Humans | Click here for the protein sequence (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=266221) of Chlorotoxin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=ShowDetailView&TermToSearch=17335414&ordinalpos=5&itool=EntrezSystem2.PEntrez.Pubmed.Pubmed_ResultsPanel.Pubmed_RVDocSum)]

Chlorotoxin (CTX) is a neurotoxin comprising 36 amino acids and is isolated from the venom of Leiurus quinquestriatus, a scorpion of the Buthidae family. A characteristic feature of the peptide is the four disulfide bonds that give it a tight tertiary structure and a single tyrosine residue that can be iodinated. Originally, CTX was described as a calcium channel blocker (1). Later, selective and specific binding of CTX to glioma cells was demonstrated by immunochemical techniques, and radiolabeled CTX was shown to bind only to tumor cells in a mouse xenograft glioma tumor model (1). On the basis of in vitro studies, CTX was discovered to bind only to malignant (glioma) and not normal (glial) cells, indicating that the toxin had a binding specificity for embryologically related tumors, particularly those of neuroectodermal origin (2). Using a recombinant form of the toxin, it was shown that CTX binds to and reduces the activity of a matrix metalloproteinase (MMP) that is associated with and indirectly regulates functioning of the chloride channels on cell membranes (3, 4). Deshane et al. showed that isoform 2 of the MMP (MMP2) was the specific cellular receptor for CTX and that the ligand did not bind to the other MMPs also expressed on the glioma cells (4). In other in vitro studies it was shown that CTX reduced the migration ability of glioma cells through tight extracellular spaces in the brain tissue by inhibition of the MMP2, because this prevented the cells from shrinking and releasing from the extracellular matrix (5).

The MMP2 enzyme activity was observed to be significantly elevated in malignant glioma cells compared to low-grade glioma and normal brain tissues, and the upregulation correlated with the malignant progression of human gliomas in vivo (6). In the same study, which used immunohistochemical techniques, MMP2 was shown to be localized only in the cells and vasculature of malignant glioma tumors. These observations explained the specificity and selectivity of CTX binding to the malignant glioma tumors observed by the various investigators. Currently, resection of the tumor is the only effective treatment for glioma, but the tumor often reappears at the same spot or close to it because not all neoplastic cells can be completely removed during surgery.

Because of its specificity and selectivity for glioma cells, a synthetic version of CTX, TM-601, was generated either by production in Escherchia coli or by chemical synthesis (2, 4, 7). The peptide has been radiolabeled with radioactive iodine (^131^I) to obtain ^131^I-TM601 and used for preclinical and clinical imaging and radiotherapy of malignant glioma (8, 9). The iodinated peptide is currently being evaluated in clinical trials (http://www.clinicaltrials.gov/ct/search;jsessionid=984B9FFECC1840A9E42C96520F968618?term=TM-601) in the United States for the treatment of solid tumors or recurrent high-grade gliomas in humans (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131I-TM-601)]

Three different methods are available for the production of CTX. This neurotoxin can either be isolated from L.quinquestriatus venom, or it may be produced and purified from E. coli by recombinant DNA and protein purification techniques (4, 7). A synthetic peptide version of CTX (TM-601) is available commercially (2). CTX is also available commercially as a freeze dried product,

Purification of CTX from scorpion venom was described by DeBin et al. (7). Crude venom was dispersed in deionized water using a Potter-Elvehjem tissue grinder. Insoluble materials in the suspension were removed by centrifugation, and the soluble portion was saved for further processing. The solution was filtered through a 10-kDa cut-off filter by centrifugation, and the filtrate was collected, vacuum-centrifuged, and reconstituted in trifluoroacetic acid (TFA). The TFA solution was batch-purified on a Waters C18 Sep-Pak cartridge, and the active component was eluted in TFA-containing acetonitrile, vacuum-centrifuged to dryness, and reconstituted in TFA for reverse-phase high-pressure liquid chromatography (RP-HPLC). All preparative RP-HPLC was performed on a Vydac TP-54 C18 column for batch purification of the various peptides. The peptides purified with RP-HPLC were repurified by ion-exchange HPLC on a polysulfoethyl aspartamide cation-exchange column, and the CTX peptide was eluted with a linear gradient of sodium chloride in phosphate buffer that contained acetonitrile (pH 4.0). Only fractions containing the center of the peaks that showed biological activity were pooled and retained from the various HPLC runs. The investigators did not provide a purification table for the scheme, and the final yield of purified CTX is not available in the publication.

For the production and purification of CTX in E. coli, a recombinant, polyhistidine (polyHis)-linked peptide (HIS-CTX) was produced (4). To produce HIS-CTX, the CTX was cloned into a pGHBE plasmid and then subcloned into a commercially available pRSETB vector that contains the N-terminal polyHis tag used for purification of the recombinant peptide. The polyHis-tagged peptide was purified by metal affinity chromatography under buffer conditions as described by the manufacturer.

The synthetic peptide version of CTX has been used in some studies (2). The peptide is available commercially from several vendors.

Some investigators have used a lyophilized preparation of the peptide for their studies (9, 10). Recombinant CTX expressed in E. coli and purified by HPLC is available commercially as a lyophilized powder.

The radiolabeling of CTX with ^131^I was described by Hockaday et al. (9), who used lyophilized CTX and followed the Iodogen method (11). Labeling of the peptide was determined by instant thin-layer chromatography. The investigators did not provide data detailing the Rf value of the ^131^I-CTX under these conditions, nor did they provide specific activity or yield of the labeling reaction. However, they mentioned that a labeling efficiency of >92% was required for use in humans. Shen et al. (8) labeled CTX with ^131^I as mentioned above and purified it on a Dowex column. They reported that the amount of free labeled iodine (^125^I or ^131^I) in the product was <5%, as determined by thin-layer chromatography. The preparations typically had a specific activity of 7.4 MBq/nM (200 µCi/nM), but the radiochemical yield was not mentioned.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131I-TM-601+in+vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131I-TM-601+rodentia)]

A study to determine the dosimetery of ^131^I-CTX in athymic mice with intracranially implanted human glioma xenografts was performed by Shen et al. (8). The investigators used ^125^I-CTX as a surrogate radiochemical to study its tissue distribution in the animals. For this, athymic mice were implanted with D54 MG human malignant glioma xenografts in the right brain. Fifteen days after implantation, the mice were intracranially injected with ^125^I-CTX in the right brain and sacrificed at 24, 48, 72, or 96 h after the injection. Subsequently, the blood, heart, stomach, small intestine, spleen, kidneys, liver, and thyroid of these animals were collected and weighed, and the radioactivity accumulation in each organ was determined. The ^125^I-CTX accumulated primarily in the tumors, but the radiochemical was also detected in the stomach, kidneys, and thyroid of the animals. Concentrations of the radiolabel decreased in all organs except the stomach and thyroid. The investigators suggested that the radioactivity was detected in the stomach and thyroid probably as a result of accumulated radiolabel from dehalogenation of the radiochemical. The kidneys accumulated the radiolabel because of rapid clearance through the urinary system. Data obtained from this study was also used to estimate doses to be used in a clinical trial for patients with malignant gliomas. Details of how this was done are given in the publication (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131-TM-601+Non-Primate+Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131-TM-601+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131-TM-601+Human+)]

A phase I/II clinical trial was performed in adult patients with recurrent high-grade glioma to investigate the biodistribution and toxicity of ^131^I-CTX (9). A lyophilized preparation of CTX was used to generate the ^131^I-labeled peptide used in this study. Patients underwent tumor resection, and an intracavitary reservoir was implanted to deliver a single dose of the radiochemical 2 to 4 weeks after the surgery. Total-body planar gamma imaging and whole-brain single-photon emission computed tomography scans were performed at 0, 1, 2, 3, and 6 to 8 days after administration of the radiochemical. Unbound ^131^I was eliminated from the brain within 48 h and the remaining radioactivity remained bound to the tumor for 6 to 8 days. A comparison of the tumor volumes, as determined by imaging and magnetic resonance imaging (MRI), indicated that tumor volumes determined with ^131^I-CTX closely paralleled the T2 volumes but not the T1-weighted gadolinium contrast volumes obtained with MRI. Similar results obtained with MRI and radiolabeling indicated that the labeled peptide was present in the tumor vicinity up to 7 days after injection. From these observations the investigators concluded that ^131^I-CTX was a suitable radiochemical to determine the extent of a primary malignant glioma.

During the study it was observed that the radiolabel rapidly penetrated the cavity wall and ~79% of the radioactivity left the site of administration within 24 h (10). The remaining label was localized primarily in the tumor cavity and some label was detected in the surrounding regions, indicating that the peptide bound tightly to the tumor. The amount of label that accumulated in the stomach, spleen, and kidneys was low, but some accumulation was observed in the bladder. This was probably because the excretion route of the ^131^I-CTX metabolites is through the urinary tract. Compared to other organs, some uptake of ^131^I-CTX by the thyroid gland was evident, but it was below toxic levels because the patients had already received a high dose of potassium iodide 1 day prior to and 3 days after administration of the radiopeptide. The investigators concluded that ^131^I-CTX may have an anti-tumoral effect and recommended that a phase II study should be conducted to confirm its efficacy.

## References

1 Soroceanu L., Gillespie Y., Khazaeli M.B., Sontheimer H. (1998). Use of chlorotoxin for targeting of primary brain tumors. Cancer Res.
2 Lyons S.A., O'Neal J., Sontheimer H. (2002). Chlorotoxin, a scorpion-derived peptide, specifically binds to gliomas and tumors of neuroectodermal origin. Glia.
3 Soroceanu L., Manning T.J., Sontheimer H. (1999). Modulation of glioma cell migration and invasion using Cl(-) and K(+) ion channel blockers. J Neurosci.
4 Deshane J., Garner C.C., Sontheimer H. (2003). Chlorotoxin inhibits glioma cell invasion via matrix metalloproteinase-2. J Biol Chem.
5 McFerrin M.B., Sontheimer H. (2006). A role for ion channels in glioma cell invasion. Neuron Glia Biol.
6 Sawaya R.E., Yamamoto M., Gokaslan Z.L., Wang S.W., Mohanam S., Fuller G.N., McCutcheon I.E., Stetler-Stevenson W.G., Nicolson G.L., Rao J.S. (1996). Expression and localization of 72 kDa type IV collagenase (MMP-2) in human malignant gliomas in vivo. Clin Exp Metastasis.
7 DeBin J.A., Maggio J.E., Strichartz G.R. (1993). Purification and characterization of chlorotoxin, a chloride channel ligand from the venom of the scorpion. Am J Physiol.
8 Shen S., Khazaeli M.B., Gillespie G.Y., Alvarez V.L. (2005). Radiation dosimetry of 131I-chlorotoxin for targeted radiotherapy in glioma-bearing mice. J Neurooncol.
9 Hockaday D.C., Shen S., Fiveash J., Raubitschek A., Colcher D., Liu A., Alvarez V., Mamelak A.N. (2005). Imaging glioma extent with 131I-TM-601. J Nucl Med.
10 Mamelak A.N., Rosenfeld S., Bucholz R., Raubitschek A., Nabors L.B., Fiveash J.B., Shen S., Khazaeli M.B., Colcher D., Liu A., Osman M., Guthrie B., Schade-Bijur S., Hablitz D.M., Alvarez V.L., Gonda M.A. (2006). Phase I single-dose study of intracavitary-administered iodine-131-TM-601 in adults with recurrent high-grade glioma. J Clin Oncol.
11 Woltanski K.P., Besch W., Keilacker H., Ziegler M., Kohnert K.D. (1990). Radioiodination of peptide hormones and immunoglobulin preparations: comparison of the chloramine T and iodogen method. Exp Clin Endocrinol.